# [Carbonyl-^11^C](S)-3-chloro-4-(4-((2-(pyridine-3-yl)pyrrolidin-1-yl)methyl)phenoxy)benzamide

Chemical name: | [Carbonyl-^11^C](S)-3-chloro-4-(4-((2-(pyridine-3-yl)pyrrolidin-1-yl)methyl)phenoxy)benzamide
Abbreviated name: | [^11^C]LY2795050
Synonym:
Agent category: | Compound
Target: | Kappa (κ) opioid receptors (KOR)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human Primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20LY2795050)]

Opioids such as morphine are commonly used analgesics in clinical practice. Three opioid receptors that mediate opioid effects have been identified with molecular cloning: delta, δ (enkephalin-preferring); kappa, κ (dynorphin-preferring); and mu, µ (ß-endorphin–preferring) (1). Each type of opioid receptor consists of subtypes of receptors as suggested by pharmacological studies (2, 3). These receptors have high specificity in both the central and peripheral nervous systems, and their presence is ubiquitous. The opioid receptors (G-protein–coupled; decrease adenylyl cyclase activity) play an important role in the regulation of analgesia, shock, appetite, thermoregulation, cardiovascular, and mental and endocrine function (2-5). Although µ opioid receptors are the major receptor to mediate the analgesic effects of opioids, κ opioid receptors (KOR) and δ opioid receptors are also important in antinociception. Opioids have been found to protect cells from ischemia injury in the heart and brain via the δ receptors. On the other hand, the κ antagonist prevents neurodegeneration.

In humans, the κ_1_ and κ_2_ KORs are the most abundant brain opioid receptors and are widely distributed in deeper layers of the neocortex (particularly temporal, parietal, and frontal cortices), striatum, and thalamus, with lower levels in the amygdala, hippocampus, occipital cortex, and cerebellum (6, 7). The KORs have been implicated in several clinical brain disorders, including substance abuse (8), epilepsy (9), Tourette’s syndrome (10), and Alzheimer’s disease (11).

(±)-4-Methoxycarbonyl-2-[1-pyrrolidinylmethyl]-1-[(3,4-dichlorophenyl)acetyl]-piperidine (GR89696) is a novel, highly potent, and selective KOR agonist (12). The (–)-isomer, (–)-4-methoxycarbonyl-2-[1-pyrrolidinylmethyl]-1-[(3,4-dichlorophenyl)acetyl]-piperidine, also known as GR103545, is the more potent optical isomer of GR89696 (IC_50_, 0.018 nM versus 6.0 nM, respectively). GR89696 is centrally penetrating, with a log P value of 3.14, and it has potent antinociceptive, sedative, and diuretic effects. The K_i_ values for GR89696 κ_1_- and κ_2_-receptor binding are in the low nanomolar or subnanomolar range. GR89696 is an agonist for the κ_2_ opioid receptor and an antagonist for the κ_1_ receptor in the guinea pig hippocampus (13). [^11^C]GR103545 was studied as a positron emission tomography (PET) agent for use with the noninvasive study of κ opioid receptors in the brain. However, there is a need for KOR antagonist radioligands because they tend to bind to both high- and low-affinity receptors (14). Hence, antagonists bind to a higher number of receptors than the agonists (15). (S)-3-Chloro-4-(4-((2-(pyridine-3-yl)pyrrolidin-1-yl)methyl)phenoxy)benzamide (LY2795050) was determined to be a selective KOR antagonist. Zheng et al. (16) prepared and evaluated [carbonyl-^11^C]LY2795050 ([^11^C]LY2795050) for use with in vivo PET imaging of KOR distribution in monkey brain tissue.

### Related Resource Links:

- Chapters in MICAD (kappa opioid receptors (http://www.ncbi.nlm.nih.gov/books?term=Kappa%20opioid%20receptor%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (kappa opioid receptors (http://www.ncbi.nlm.nih.gov/gene/4986))
- Articles in Online Mendelian Inheritance in Man (OMIM) (kappa opioid receptors (http://omim.org/entry/165196))
- Clinical trials (kappa opioid receptors (http://www.clinicaltrials.gov/ct2/results?term=Kappa+opioid+AND+receptor))
- Drug information in FDA (kappa opioid receptors (http://google2.fda.gov/search?q=kappa+opioid+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20LY2795050%20and%20synthesis)]

Zheng et al. (16) reported a two-step synthesis of [^11^C]LY2795050 by reaction of the corresponding iodophenyl precursor ((S)-3-(1-(-4-(2-chloro-4-iodophenoxy)benzyl(pyrrolidin-2-yl)pyridine))) with H[^11^C]CN in the presence of K_2_CO_3_ and Pd_2_dba_3_ in dimethylformamide for 5 min at 80°C, followed by hydrolysis with addition of NaOH and H_2_O_2_ to yield [^11^C]LY2795050. [^11^C]LY2795050 was purified with high-performance liquid chromatography (HPLC), with >99% radiochemical and enantiomeric purity. The average yield was 12% at end of synthesis, with a total synthesis time of 45 min. The average specific activity (n = 16) was 23.68 GBq/μmol (640 mCi/μmol) at end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20LY2795050%20and%20in%20vitro)]

Zheng et al. (16) performed in vitro competition binding assays with cloned human opioid receptors. LY2795050 exhibited K_i_ values of 0.72, 25.8, and 153 nM for the κ, µ, and δ opioid receptors, respectively. LY2795050 exhibited only antagonistic activity in all three opioid receptor functional assays.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20LY2795050%20and%20rodentia)]

Ex vivo biodistribution studies in normal rats (n = 4) injected with 3 μg/kg unlabeled LY2795050 were performed by Zheng et al. (16). LY2795050 brain tissue concentrations were determined with mass spectrometry-HPLC at 10, 20, 40, and 60 min after intravenous injection. There was a rapid accumulation in the striatum and cerebellum, followed by a fast washout. The concentrations in the striatum were 4.0, 2.0, 0.8, and 0.5 ng/g at 10, 20, 40, and 60 min, respectively. The striatum/cerebellum ratios were 2 and 2.5 at 10 min and 60 min, respectively. Zheng et al. (16) performed ex vivo distribution studies in the striatum and cerebellum of wild-type (WT) and KOR-knockout (κ-KO) mice. LY2795050 concentrations were 3.0 ± 0.6 ng/g (n = 9) and 0.6 ± 0.2 ng/g (n = 8) in the striatum of WT and κ-KO mice (P < 0.05), respectively. On the other hand, the ligand concentrations were similar in the cerebellum of WT (1.0 ± 0.6 ng/g ) and κ-KO (0.7 ± 0.2 ng/g ) mice. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20LY2795050%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20LY2795050%20%28primate%20not%20human%29)]

Zheng et al. (16) studied three rhesus monkeys with [^11^C]LY2795050 PET imaging under baseline conditions and after pretreatment with naloxone (1 mg/kg), an opioid receptor competitive antagonist, or co-injection of the selective KOR antagonist LY2456302 (0.01–0.3 mg/kg). There was a heterogeneous distribution of radioactivity in the brain, with the highest levels in the basal ganglia and cingulate cortex and the lowest level in the cerebellum. Regional brain accumulation peaked within 20 min. Regional total distribution volume (V_T_) values and binding potential (BP_ND_) were derived using the arterial input function and a two-tissue-compartment model (2TCM). High levels of [^11^C]LY2795050 radioactivity were found in the globus pallidus (V_T_ = 5.2 ± 1.4 ml/g), putamen (V_T_ = 4.2 ± 0.5 ml/g), substantia nigra (V_T_ = 3.8 ± 1.4 ml/g), and cingulate cortex (V_T_ = 3.7 ± 1.4 ml/g). Intermediate levels were found in the insula (V_T_ = 3.4 ± 1.0 ml/g), caudate (V_T_ = 3.0 ± 1.4 ml/g), frontal cortex (V_T_ = 3.0 ± 1.1 ml/g), and temporal cortex (V_T_ = 2.8 ± 0.9 ml/g). Low levels were found in the cerebellum (V_T_ = 2.4 ± 0.6 ml/g). Pretreatment with naloxone revealed that the specific binding values for [^11^C]LY2795050 were reduced in all regions to the level of the cerebellum. BP_ND_ values of these brain regions determined with the 2TCM were similar to those determined with the simplified reference tissue model. There was a dose-dependent inhibition of radioactivity in the brain with LY2456302, with 50% inhibition of the [^11^C]LY2795050 binding dose of 0.028 mg/kg.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20LY2795050%20and%20human)]

No publication is currently available.

## References

1 Minami M., Satoh M. (1995). Molecular biology of the opioid receptors: structures, functions and distributions. Neurosci Res.
2 Satoh M., Minami M. (1995). Molecular pharmacology of the opioid receptors. Pharmacol Ther.
3 Waldhoer M., Bartlett S.E., Whistler J.L. (2004). Opioid receptors. Annu Rev Biochem.
4 Molina P.E. (2006). Opioids and opiates: analgesia with cardiovascular, haemodynamic and immune implications in critical illness. J Intern Med.
5 Barry U., Zuo Z. (2005). Opioids: old drugs for potential new applications. Curr Pharm Des.
6 Hiller J.M., Fan L.Q. (1996). Laminar distribution of the multiple opioid receptors in the human cerebral cortex. Neurochem Res.
7 Peckys D., Landwehrmeyer G.B. (1999). Expression of mu, kappa, and delta opioid receptor messenger RNA in the human CNS: a 33P in situ hybridization study. Neuroscience.
8 Mello N.K., Negus S.S. (2000). Interactions between kappa opioid agonists and cocaine. Preclinical studies. Ann N Y Acad Sci.
9 de Lanerolle N.C., Williamson A., Meredith C., Kim J.H., Tabuteau H., Spencer D.D., Brines M.L. (1997). Dynorphin and the kappa 1 ligand [3H]U69,593 binding in the human epileptogenic hippocampus. Epilepsy Res.
10 Chappell P.B., Leckman J.F., Scahill L.D., Hardin M.T., Anderson G., Cohen D.J. (1993). Neuroendocrine and behavioral effects of the selective kappa agonist spiradoline in Tourette's syndrome: a pilot study. Psychiatry Res.
11 Mathieu-Kia A.M., Fan L.Q., Kreek M.J., Simon E.J., Hiller J.M. (2001). Mu-, delta- and kappa-opioid receptor populations are differentially altered in distinct areas of postmortem brains of Alzheimer's disease patients. Brain Res.
12 Birch P.J., Rogers H., Hayes A.G., Hayward N.J., Tyers M.B., Scopes D.I., Naylor A., Judd D.B. (1991). Neuroprotective actions of GR89696, a highly potent and selective kappa-opioid receptor agonist. Br J Pharmacol.
13 Caudle R.M., Mannes A.J., Iadarola M.J. (1997). GR89,696 is a kappa-2 opioid receptor agonist and a kappa-1 opioid receptor antagonist in the guinea pig hippocampus. J Pharmacol Exp Ther.
14 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
15 Ginj M., Zhang H., Waser B., Cescato R., Wild D., Wang X., Erchegyi J., Rivier J., Macke H.R., Reubi J.C. (2006). Radiolabeled somatostatin receptor antagonists are preferable to agonists for in vivo peptide receptor targeting of tumors. Proc Natl Acad Sci U S A.
16 Zheng M.Q., Nabulsi N., Kim S.J., Tomasi G., Lin S.F., Mitch C., Quimby S., Barth V., Rash K., Masters J., Navarro A., Seest E., Morris E.D., Carson R.E., Huang Y. (2013). Synthesis and Evaluation of 11C-LY2795050 as a kappa-Opioid Receptor Antagonist Radiotracer for PET Imaging. J Nucl Med.